# GPI-78

Chemical name: | GPI-78
Abbreviated name:
Synonym:
Agent Category: | Compound
Target: | Prostate-specific membrane antigen (PSMA), or N-acetyl α-linked acidic dipeptidase (NAALADase)
Target Category: | Enzyme inhibitor
Method of detection: | Optical, near-infrared fluorescence
Source of signal: | IRDye78
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=IRDye78%5BAll%20Fields%5D)]

Optical fluorescence imaging is increasingly used to study the biological functions of specific targets in vitro and in small animals (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when visible light-absorbing (350-700 nm) fluorophores are used because of high tissue absorption and scatter. Use of near-infrared (NIR) fluorescence (700-900 nm) for detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic ranges and minimal background as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alterative to radionuclide imaging in vitro and in small animals.

IRDye78 is a heptamethine indocyanine-type NIR fluorophore with peak absorption at 772 nm and peak emission at 790 nm (3). It provides a quantum yield of 9.0% and has a molecular mass of 1,083 Da. IRDye78 N-hydroxysuccinimide (NHS) ester can be conjugated to antibodies and low-molecular-weight ligands with one or more free primary amines.

Prostate-specific membrane antigen (PSMA) is a unique type II, transmembrane-bound glycoprotein that is overexpressed on prostate tumor cells and in the neovasculature of most solid prostate tumors but not in the vasculature of normal tissues (4, 5). This unique expression of PSMA makes it an important biomarker as well as a large extracellular target of imaging agents. PSMA was found to have N-acetyl α-linked acidic dipeptidase (NAALADase, or glutamate carboxypeptidase II) activity (6). PGI is a small molecule that is a potent inhibitor of NAALADase, with a K_i_ of 9.0 nM, whereas IRDye78 had a K_i_ of 500 nM (7). On the other hand, GPI-78 had a K_i_ of 0.4 nM. GPI-78 is being developed as an optical agent for imaging prostate cancer.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28GPI%5BAll%20Fields%5D%20AND%2078%5BAll%20Fields%5D%29%20AND%20synthesis%5BAll%20Fields%5D)]

Humblet et al. (7) reported the synthesis of GPI-78 by reaction of IRDye78 monofunctional NHS ester with the single primary amino group of GPI. GPI-78 was purified by reverse-phase high-performance liquid chromatography, and its identity was confirmed by mass spectroscopy with >95% purity. GPI-78 had peak absorption at 773 nm and peak emission at 792 nm. The conjugation yields were 60%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GPI-78%20and%20in%20vitro)]

Humblet et al. (7) determined that the dissociation constant (K_d_) for GPI-78 binding to the active site of PSMA, as measured by fluorescence polarization, was 0.84 ± 0.15 nM. This value is very similar to the K_i_ (0.43 ± 0.04 nM) determined in enzymatic assays, suggesting that GPI-78 is binding to the active site.

GPI-78 bound to PSMA-negative PC-3 human prostate cancer cells overexpressing PSMA, but not to Erb-B2-overexpressing PC-3 cells (7). GPI-78 also bound to PSMA-positive LNCaP human cancer cells. There was 50% more fluorescent signal when the cells were incubated at 37 °C versus 4 °C because PSMA was being internalized at 37 °C. Experiments in which LNCaP cells were incubated with 2 μM GPI-78 at 4 °C for 20 min indicated that there were about 3.2 × 10^5^ receptor sites per cell.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GPI-78%20and%20rodentia)]

Nude mice bearing PSMA-positive LNCaP (NAALADase activity = 10 pmol/min/mg) cells on the right flank and PSMA-negative human bladder cancer TsuPRI cells (NAALADase activity = 0 pmol/min/mg) on the left flank received injections containing 5 nmol of GPI-78 or IRDye78 (7). Both IRDye78 and GPI-78 (injected intravenously) were cleared rapidly from the blood with similar half-lives: the early phase was 1.6 and 1.5 min and the late phase was 3.4 and 2.3 min, respectively. There was a rapid increase in signal intensities in the skin and kidney, reaching a plateau by 5 min with a gradual washout over a few hours. The peak GPI-78 tumor/background ratios were 1.80 ± 0.21 and 1.20 ± 0.05 (P = 0.024) for PSMA-positive and PSMA-negative tumors, respectively. The peak IRDye78 tumor/background ratios were 1.20 ± 0.11 and 1.30 ± 0.21 (P = 0.7) for PSMA-positive and PSMA-negative tumors, respectively. In vivo imaging of the tumors, performed with a small-animal NIR fluorescence imaging system, revealed that only PSMA-positive tumors exhibited any signal above background, with a brighter signal from GPI-78 than IRDye78.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GPI-78%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GPI-78%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=GPI-78%20and%20human)]

No publication is currently available.

## NIH Support

CA88245

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Nakayama A., del Monte F., Hajjar R.J., Frangioni J.V. (2002). Functional near-infrared fluorescence imaging for cardiac surgery and targeted gene therapy. Mol Imaging.
4 Feneley M.R., Jan H., Granowska M., Mather S.J., Ellison D., Glass J., Coptcoat M., Kirby R.S., Ogden C., Oliver R.T., Badenoch D.F., Chinegwundoh F.I., Nargund V.H., Paris A.M., Britton K.E. (2000). Imaging with prostate-specific membrane antigen (PSMA) in prostate cancer. Prostate Cancer Prostatic Dis.
5 Ghosh A., Heston W.D. (2004). Tumor target prostate specific membrane antigen (PSMA) and its regulation in prostate cancer. J Cell Biochem.
6 Luthi-Carter R., Barczak A.K., Speno H., Coyle J.T. (1998). Molecular characterization of human brain N-acetylated alpha-linked acidic dipeptidase (NAALADase). J Pharmacol Exp Ther.
7 Humblet V., Lapidus R., Williams L.R., Tsukamoto T., Rojas C., Majer P., Hin B., Ohnishi S., De Grand A.M., Zaheer A., Renze J.T., Nakayama A., Slusher B.S., Frangioni J.V. (2005). High-affinity near-infrared fluorescent small-molecule contrast agents for in vivo imaging of prostate-specific membrane antigen. Mol Imaging.